# [^123^I/^125^I]6-Iodo-2-(4´-dimethylamino)-phenyl-imidazo[1,2-a]pyridine

Chemical name: | [^123^I/^125^I]6-Iodo-2-(4´-dimethylamino)-phenyl-imidazo[1,2-a]pyridine
Abbreviated name: | [^123^I]IMPY or [^125^I]IMPY, IMPY
Synonym:
Agent Category: | Compound
Target: | Aggregates of β-amyloid (Aβ) peptides
Target Category: | Acceptor binding
Method of detection: | SPECT
Source of signal: | ^123^I,^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28123I%29IMPY%20OR%20%28125I%29IMPY)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1, 2). It is characterized by the presence, in the brain, of senile plaques of β-amyloid (Aβ) peptides with intracellular neurofibrillary tangles of filaments containing the hyperphosphorylated protein tau (3, 4). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD, and although the mechanisms of the disease are still not fully understood, reducing the deposition of amyloid plaques seems to benefit patients.

Several radioligands for positron emission tomography (PET) have been developed (5-7) and tested in humans as in vivo diagnostic tools for imaging and measuring the formation and Aβ deposits (7). The first successful agent used in human studies was 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malononitrile ([^18^F]FDDNP) (8), a malonitrile derivative found to bind to both neurofibrillary tangles and Aβ plaques. The second successful attempt in humans was made with [^11^C]PIB (9), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1. [^11^C]PIB showed marked retention in areas of association cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand tested in humans was [^11^C]4-N-methylamino-4´-hydroxystilbene, a stilbene derivative commonly named [^11^C]SB-13. SB-13 was also synthesized and labeled with either I-123 or C-11 for in vivo imaging using PET.

The radioiodinated ligand 6-iodo-2-(4´-dimethylamino)-phenyl-imidazo[1,2-a]pyridine ([^125^I]IMPY or [^123^I]IMPY), is a novel probe displaying high specific binding for Aβ plaques and very favorable brain uptake kinetics in rodents. Published research has shown that this radioligand was a good candidate for the detection of Aβ plaques in humans when used with single-photon emission computed tomography (SPECT).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28123I%29IMPY%20OR%20%28125I%29IMPY%29%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

[^125^I]IMPY or [^123^I]IMPY can be prepared by an iododestannylation reaction from the corresponding tin precursor using hydrogen peroxide as catalyst. Using this protocol, Kung et al. (10) obtained the no-carrier-added product with a high specific activity (81,400 GBq/mmol (2,200 Ci/mmol) for [^125^I]IMPY and 8,140 GBq/mol (220,000 Ci/mmol) for [^123^I]IMPY), an overall yield ranging from 30 to 45%, and a radiochemical purity greater than 95%. The method reported by the authors (10) in 2002 used a purification process that included high-pressure liquid chromatography (HPLC). The stabilities of the purified tracers (by HPLC) were 6 h at room temperature for [^123^I]IMPY and 8 weeks for [^125^I]IMPY stored in 100% ethanol at –20°C.

A simplified method was reported by Kung et al. (11) in 2004. This method improved the yield and simplified the purification process of the radioiodinated IMPY. Purification was done with a simple C_4_ mini-column with stepwise washing and elution using ethanol (3 ml at 10% and 3 ml at 20% for the washing). The radiochemical yield obtained was >50%, and the total synthesis time was less than 1 h. The radiochemical purity obtained was >95% (determined by HPLC or thin-layer chromatography).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28125I%29IMPY%20OR%20%28123I%29IMPY%29%20AND%20in%20vitro)]

In vitro binding assays using preformed synthetic Aβ40 aggregates (10) showed that [^125^I]IMPY had very good binding affinities for amyloid plaques while competing well for the thioflavin binding site recognized by [^125^I]2-(4´-dimethylaminophenyl)-6-iodobenzothiazole ([^125^I]TZDM), a selective probe for amyloid plaques studied previously (12). The inhibition coefficient (K_i_) for [^125^I]IMPY was 15 ± 5 nM (at 25 °C). Replacement of the iodine by a methyl or hydrogen appeared to substantially decrease the binding affinity of [^125^I]IMPY for Aβ aggregates (K_i_ ~242 and 1242 nM for methyl group and hydrogen, respectively).

In vitro audiography of amyloid plaques in postmortem brain sections of AD patients showed distinct labeling of the plaques after exposure to [^125^I]IMPY, whereas no specific binding of the tracer was observed in normal brains. The specificity of Aβ plaque labeling by [^125^I]IMPY was further supported by blocking experiments using a competing concentration of thioflavin-T (100 µM). In addition, when pretreated with formic acid (which destroys the ß-sheet structure), the AD brain sections showed no retention of [^125^I]IMPY (10).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28125I%29IMPY%20OR%20%28123I%29IMPY%29%20AND%20rodentia%5BMeSH%5D)]

Biodistribution studies in healthy male mice (2-3 months old; weight, 20-30 g) injected with [^125^I]IMPY (4.9 MBq (133 µCi)) showed excellent brain uptake (2.9% of the initial injected dose (ID) at 2 min post injection) and rapid washout (0.26% and 0.2% of initial ID remaining in the brain at 30 and 60 min post injection, respectively) (10). Those results indicated that [^125^I]IMPY had much more favorable in vivo kinetic properties than the other iodinated probe, [^125^I]TZDM (12).

Plaque labeling with [^125^I]IMPY was studied by Kung et al. (10) in an 18-month-old transgenic mouse (Tg2576) that produced excess amyloid plaques in the brain (10). Ex vivo autoradiograms of brain sections of the animal at 4 h after an intravenous injection of the tracer (injected dose: 4.9 MBq (133 µCi)) clearly showed distinct plaque labeling with low background activity. When the same brain section was stained with the fluorescent dye thioflavin-S, the same amyloid plaques showed prominent fluorescent labeling consistent with the results of the autoradiogram.

Zhuang et al. (13) measured the levels of radiotracer uptake (in % ID/organ) in normal mice (ICR) at 2 min, 30 min, and 2 h, respectively, and found the following values: 2.88 ± 0.25, 0.26 ± 0.00, and 0.14 ± 0.03 for the brain; 20.9 ± 2.63, 6.32 ± 0.55, and 2.90 ± 0.21 for the liver; 4.75 ± 0.49, 1.51± 0.27, and 0.53 ± 0.05 for the kidney; and 1.56 ± 0.33, 0.31 ± 0.07, and 0.20 ± 0.05 for the lung.

At 30 min after intravenous injection of 4.9 MBq (133 µCi) of [^125^I]IMPY in 14- to 16-month-old TT mice, Kung et al. (11), found that the radiotracer uptake was the highest in the cortical region (~0.9% ID/g of tissue), followed by the hippocampal (~0.8% ID/g of tissue) and cerebellar (~0.7% ID/g of tissue) regions. The lowest binding was found in the striatal region (~0.5-0.6% ID/g of tissue).

In that same research study, Kung et al. (11) investigated the effect of the carrier IMPY on several factors affecting the uptake of [^125^I]IMPY by measuring the plasma input function and brain metabolites, with or without added carrier in the injected dose. Results showed that when the carrier was co-injected with [^125^I]IMPY, degradation of [^125^I]IMPY was significantly reduced and more tracer was retained by the brains of TT mice.

At 30 min post injection, approximately 0.97 ± 0.11% ID/organ (n = 3) was present in the brain with no carrier added, whereas approximately 1.36 ± 0.05% ID/organ (n = 3) and 1.93 ± 0.09% ID/organ (n = 3) were retained with 2 and 10 mg/kg IMPY, respectively. In the blood, those values were 6.46, 7.20, and 8.48% for 0, 2, and 10 mg/kg carrier, respectively. At 2 min post injection, adding the carrier IMPY to the [^125^I]IMPY injection significantly increased the amount of nonmetabolized radiotracer in the plasma.

As proposed by Kung et al. (11) in 2004, the fact that in vivo binding of [^125^I]IMPY to amyloid plaques cannot be blocked by co-injection of the carrier may be attributable to the following: (a) the binding capacity or number of sites for [^125^I]IMPY is very high; or (b) the amount of injected carrier is limited by its solubility and therefore is not high enough to reach the minimal necessary blocking dose. As pointed out by the authors, the binding capacity of [^125^I]IMPY is clearly high in the cortex and other brain tissues affected by the disease.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28125I%29IMPY%20OR%20%28123I%29IMPY%29%20AND%20%28dog%20OR%20sheep%20OR%20rabbit%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28125I%29IMPY%20OR%20%28123I%29IMPY%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28125I%29IMPY%20OR%20%28123I%29IMPY%29%20AND%20human)]

No publication is currently available.

## References

1 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci, 11 Spec No: p. 213-328.
2 Forstl H, Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
3 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
4 Brandt R, Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
5 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
6 Bacskai BJ, Hickey GA, Skoch J, Kajdasz ST, Wang Y, Huang GF, Mathis CA, Klunk WE, Hyman BT. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
7 Wu C, Pike VW, Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
8 Shoghi-Jadid K, Small GW, Agdeppa ED, Kepe V, Ercoli LM, Siddarth P, Read S, Satyamurthy N, Petric A, Huang SC, Barrio JR. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
9 Klunk WE, Engler H, Nordberg A, Wang Y, Blomqvist G, Holt DP, Bergstrom M, Savitcheva I, Huang GF, Estrada S, Ausen B, Debnath ML, Barletta J, Price JC, Sandell J, Lopresti BJ, Wall A, Koivisto P, Antoni G, Mathis CA, Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Kung MP, Hou C, Zhuang ZP, Zhang B, Skovronsky D, Trojanowski JQ, Lee VM, Kung HF. (2002). IMPY: an improved thioflavin-T derivative for in vivo labeling of beta-amyloid plaques. Brain Res.
11 Kung MP, Hou C, Zhuang ZP, Cross AJ, Maier DL, Kung HF. (2004). Characterization of IMPY as a potential imaging agent for beta-amyloid plaques in double transgenic PSAPP mice. Eur J Nucl Med Mol Imaging.
12 Zhuang ZP, Kung MP, Hou C, Skovronsky DM, Gur TL, Plossl K, Trojanowski JQ, Lee VM, Kung HF. (2001). Radioiodinated styrylbenzenes and thioflavins as probes for amyloid aggregates. J Med Chem.
13 Zhuang ZP, Kung MP, Wilson A, Lee CW, Plossl K, Hou C, Holtzman DM, Kung HF. (2003). Structure-activity relationship of imidazo[1,2-a]pyridines as ligands for detecting beta-amyloid plaques in the brain. J Med Chem.